# ^177^Lu-Benzyl-diethylenetriamine pentaacetic acid-anti-carbonic anhydrase IX small immunoprotein A3

Chemical name: | ^177^Lu-Benzyl-diethylenetriamine pentaacetic acid-anti-carbonic anhydrase IX small immunoprotein A3
Abbreviated name: | ^177^Lu-Bn-DTPA-SIP-A3
Synonym:
Agent category: | Antibody fragment, small immunoprotein (SIP)
Target: | Carbonic anhydrase IX, hypoxia
Target category: | Enzyme
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar
Source of signal: | ^177^Lu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=94963095), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=125661057) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=55894&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about human carbonic anhydrase IX.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SIP+A3)]

In a variety of solid tumors, hypoxia has been found to lead to tumor progression and to the resistance to chemotherapy and radiotherapy (1-3). Tumor oxygenation is heterogeneously distributed within human tumors (4). Hypoxia in malignant tumors is thought to be a major factor limiting the efficacy of chemotherapy and radiotherapy. It would be beneficial to assess tumor oxygenation before and after therapy to provide an evaluation of tumor response to treatment and an insight into new therapeutic treatments (5). Tumor oxygenation is measured invasively using computerized, polarographic, oxygen-sensitive electrodes, which is regarded as the gold standard (6). Functional and non-invasive imaging of intratumoral hypoxia has been demonstrated to be feasible for the measurement of tumor oxygenation (7). This has led to the research and development of hypoxia-targeted, non-invasive markers of tumor hypoxia.

Chapman proposed the use of 2-nitroimidazole compounds for hypoxia imaging (8). 2-Nitroimidazole compounds are postulated to undergo reduction in hypoxic conditions, forming highly reactive oxygen radicals that subsequently bind covalently to macromolecules inside the cells (9). [^18^F]Fluoromisonidazole ([^18^F]FMISO) is the most widely used positron emission tomography (PET) tracer for imaging tumor hypoxia (7). Carbonic anhydrase (CA) IX is one of the most highly overexpressed genes in cells under hypoxic conditions (10). It is a transmembrane glycoprotein with CA activity in the extracellular domain, and it is found to be overexpressed in renal cell, cervical, lung, and colorectal tumors. Monoclonal antibodies have been developed for in vitro and in vivo localization of CA IX on cells (11). Recently, a bispecific A3 monoclonal antibody to CA IX was constructed by the fusion of two A3 scFv fragments to form a divalent scFv small immunoprotein (SIP-A3; molecular weight, ~80 kDa) (12). SIP-A3 was labeled with ^177^Lu via isothiocyanate-benzyl-diethylenetriamine pentaacetic acid (SCN-Bn-DTPA) to form ^177^Lu-Bn-DTPA-SIP-A3 for use in single-photon emission computed tomography (SPECT) imaging of CA IX in nude mice bearing human solid tumors.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Carbonic%20anhydrase%20IX+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Carbonic anhydrase IX (http://www.ncbi.nlm.nih.gov/gene/55894)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=CA%20IX)
- Clinical trials (Carbonic anhydrase IX (http://www.clinicaltrials.gov/ct2/results?term=CA+IX))
- Drug information in FDA (Carbonic anhydrase IX (http://google2.fda.gov/search?q=carbonic+anhydrase+IX&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=1&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SIP+A3+synthesis)]

Isothiocyanate-benzyl-DTPA and SIP-A3 (50:1 molar ratio) were incubated in 0.1 M sodium bicarbonate buffer (pH 8.2) for 1 h at room temperature (12). Benzyl-DTPA-SIP-A3 was isolated from the incubation mixture with a PD-10 column. Mass spectroscopy analysis showed ~2 DTPA molecules per SIP-A3 molecule. Benzyl-DTPA-SIP-A3 in 125 mM ammonium acetate buffer (pH 5.5) was mixed with a predetermined amount of ^177^Lu. The mixture was incubated for 1 h at room temperature with a labeling efficiency of >95%. ^177^Lu-Bn-DTPA-SIP-A3 was purified with column chromatography. The specific activity of ^177^Lu-Bn-DTPA-SIP-A3 was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SIP+A3+in+vitro)]

Ahlskog et al. (12) performed binding experiments with scFv-A3 using a Biacore sensor chip immobilized with extracellular domain of CA IX. The dissociation constant (K_d_ ) was 2.4 nM. Cytometry analysis showed a strong binding of SIP-A3 to LS174T colorectal tumor cells and a moderate binding to SK-RC-52 renal carcinoma cells. Immunofluorescence staining of various tumor sections revealed a strong binding of SIP-A3 to LS174T tumors, HT-28 colorectal carcinomas, SW 1222 colorectal carcinomas, U87 gliomas, and SK-RC-52 tumors, but not of MCF-7 breast carcinomas and Ramos lymphomas.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SIP+A3+rodentia)]

Ahlskog et al. (12) studied the biodistribution of ^177^Lu-Bn-DTPA-SIP-A3 in mice (n = 4) bearing LS174T tumors at 24 h after injection. The tracer accumulation in the LS174T tumors was 2.41 ± 0.19% injected dose per gram (ID/g). The organ with the highest radioactivity was the kidneys (85.7% ID/g), followed by the liver (11.8% ID/g), spleen (5.2% ID/g), and lung (1.0% ID/g). The tumor/blood ratio was 16.7. ^177^Lu-Bn-DTPA-SIP-HyNEL10 (anti-lysozyme) showed tumor accumulation of 1.13 ± 0.08% ID/g with a tumor/blood ratio of 12.9. The tumor accumulation of ^177^Lu-Bn-DTPA-SIP-A3 was significantly higher than that of ^177^Lu-Bn-DTPA-SIP-HyNEL10 (P < 0.001). Ex vivo immunohistochemical staining of tumors and tissues at 6 h after injection of SIP-A3 and 0.5 h after injection of pimonidazole (hypoxia staining) showed that a higher fluorescence signal was detected in the tumor lesions than in the normal tissues. There was an overlap between pimonidazole staining and SIP-A3 fluorescence signal in the tumor sections. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SIP+A3+(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SIP+A3+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SIP+A3+human)]

No publication is currently available.

## References

1 Serkies K., Jassem J. (2005). Chemotherapy in the primary treatment of cervical carcinoma. Crit Rev Oncol Hematol.
2 Vaupel P., Mayer A. (2005). Hypoxia and anemia: effects on tumor biology and treatment resistance. Transfus Clin Biol.
3 Rajendran J.G., Krohn K.A. (2005). Imaging hypoxia and angiogenesis in tumors. Radiol Clin North Am.
4 Vaupel P., Harrison L. (2004). Tumor hypoxia: causative factors, compensatory mechanisms, and cellular response. Oncologist.
5 Dehdashti F., Grigsby P.W., Mintun M.A., Lewis J.S., Siegel B.A., Welch M.J. (2003). Assessing tumor hypoxia in cervical cancer by positron emission tomography with 60Cu-ATSM: relationship to therapeutic response-a preliminary report. Int J Radiat Oncol Biol Phys.
6 Raleigh J.A., Dewhirst M.W., Thrall D.E. (1996). Measuring Tumor Hypoxia. Semin Radiat Oncol.
7 Foo S.S., Abbott D.F., Lawrentschuk N., Scott A.M. (2004). Functional imaging of intratumoral hypoxia. Mol Imaging Biol.
8 Chapman J.D. (1979). Hypoxic sensitizers--implications for radiation therapy. N Engl J Med.
9 Chapman J.D., Baer K., Lee J. (1983). Characteristics of the metabolism-induced binding of misonidazole to hypoxic mammalian cells. Cancer Res.
10 Loncaster J.A., Harris A.L., Davidson S.E., Logue J.P., Hunter R.D., Wycoff C.C., Pastorek J., Ratcliffe P.J., Stratford I.J., West C.M. (2001). Carbonic anhydrase (CA IX) expression, a potential new intrinsic marker of hypoxia: correlations with tumor oxygen measurements and prognosis in locally advanced carcinoma of the cervix. Cancer Res.
11 Lam J.S., Pantuck A.J., Belldegrun A.S., Figlin R.A. (2005). G250: a carbonic anhydrase IX monoclonal antibody. Curr Oncol Rep.
12 Ahlskog J.K., Schliemann C., Marlind J., Qureshi U., Ammar A., Pedley R.B., Neri D. (2009). Human monoclonal antibodies targeting carbonic anhydrase IX for the molecular imaging of hypoxic regions in solid tumours. Br J Cancer.